# Gadobutrol

Chemical name: | Gadobutrol
Abbreviated name: | Gd-DO3A-butrol
Synonym: | [1,4,7-Tris(carboxymethyl)-10-(1-(hydroxymethyl)-2,3-dihydroxypropyl)-1,4,7,10-tetraazacyclododecanato] gadolinium(III); Gadovist^®^; 10-[(1SR,2RS)-2,3-dihydroxy-1-hydroxymethylpropyl]-1,4,7,10-tetraazacyclodecane-1,4,7-triacetic acid, gadolinium; Gd-BT-DO3A; Gd^3+^-10-(2,3-dihydroxy-1-hydroxymethylpropyl)-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid; Gadolinium, (10-(2,3-Dihydroxy-1-(hydroxymethyl)propyl)-1,4,7,10-tetraazacyclodecane-1,4,7-triacetato(3-)-N1,N4,N7,N10,O1,O4,O7)-
Agent Category: | Compound
Target: | Nontargeted, blood pool, extracellular fluid space
Target Category: | Nonspecific filling of extracellular fluid space
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium (Gd)
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gadobutrol%20OR%20Gd-DO3A-butrol%20OR%20Gadovist%29)]

Gadobutrol (Gd-DO3A-butrol) is a nonionic, paramagnetic contrast agent developed for tissue contrast enhancement in magnetic resonance imaging (MRI) (1-3).

Water-soluble paramagnetic contrast agents are generally metal chelates with unpaired electrons, and they work by shortening both the T_1_ and T_2_ relaxation times of surrounding water protons to produce the signal-enhancing effect (1, 2, 4). At normal clinical doses of 0.1-0.2 mmol/kg, the T_1_ effect tends to dominate. Current agents are water-soluble compounds that distribute in the extracellular fluid and do not cross the intact blood-brain barrier (BBB). They are often used to enhance signals of central nervous system (CNS) tissues that lack a BBB (e.g., pituitary gland), extraaxial tumors (e.g., meningiomas), and areas of BBB breakdown (e.g., tumor margins). In these cases, small or multiple CNS lesions are more clearly delineated with contrast enhancement. In addition, contrast enhancement can highlight vasculature, delineate the extent of disease, and confirm the impression of normal or nonmalignant tissues. These contrast agents can also be used in a similar nonspecific manner to enhance contrast between pathologies and surrounding normal areas in other organs (1, 2, 5).

Gadolinium(III) (Gd^3+^), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective at enhancing proton relaxation because of its high magnetic moment and very labile water coordination (2, 6-9). Gadopentetate dimeglumine (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical efficacy, patient safety and patient tolerance. The major chemical differences among these Gd chelates or Gd-based contrast agents (GBCAs) are the presence or absence of overall charge, ionic or nonionic, and their ligand frameworks (linear or macrocyclic). Gd-DO3A-butrol has a macrocyclic framework and is neutral (10, 11). The DO3A-butrol ligand was developed based on the belief that high overall hydrophilicity of an agent is generally associated with very low protein binding and good biological tolerance (12). It is a modification of the Gd-DO3A compound in which a trihydroxybutyl group is attached to the macrocyclic ligand to ensure high hydrophilicity. The ligand contains two chiral carbons at C-13 and C-14, therefore, the product is a racemic mixture of (13R, 14S)− and (13S, 14R)−. The Gd(III) in Gd-DO3A-butrol has a coordination number of 9. Gd-DO3A-butrol is a water-soluble, highly hydrophilic compound with a partition coefficient between n-butanol and buffer at pH 7.6 of ~ 0.006 (13).

Gd-DO3A-butrol is not commercially available in the United States, but it is commercially available in Canada at a concentration of 1.0 mmol/ml (604.72 mg/ml) for contrast enhancement during cranial and spinal imaging with MRI and MR angiography. At this concentration, it has an osmolarity of 1117 mOsm/kg at 37 ºC, viscosity of 4.96 mPa at 37 ºC, and log P(n-octanol/water) of −5.4 at 25 ºC.

Both renal and extra-renal toxicities have been reported following the clinical use of gadolinium in patients with underlying kidney disease (14-16). In 2007, the US FDA (http://www.fda.gov/cder/drug/infopage/gcca/default.htm) requested manufacturers of all GBCAs to add new warnings about exposure to GBCAs increases the risk for nephrogenic systemic fibrosis (NSF) in patients with advanced kidney disease.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gadobutrol%20or%20Gd-DO3A-butrol%20or%20Gadovist%29%20AND%20synthesis)]

Vogler et al. (17) discussed the general method for preparing the macrocyclic core based on the Richman-Atkins method. In this method, 5-amino-2,2-dimethyl-6-hydroxy-1,3-dioxepan was treated with tosyl aziridine to give 1,7-ditoxyl-4-(6-hydroxy-2,2-dimethyl-1,3-dioxepan-5-yl)-1,4,7-triazaheptane. This compound was deprotonated with sodium ethoxide and reacted with the tritosylate of diethanolamine to give a macrocyclic intermediate. It was then treated with lithium in liquid ammonia to remove the tosyl groups to give a mono-substituted tetramine, which was then alkylated with chloroacetic acid at pH 9-10. DO3A-butrol was produced by a final treatment with diluted hydrochloric acid. The ligand was reacted with gadolinium oxide in water at 90 ºC to produce Gd-DO3A-butrol.

Platzek et al. (12) described three approaches to synthesizing the DO3A-butrol ligand. One approach was preferred because it involved fewer steps and allowed scaled up production for clinical applications. In this approach, 1-(1-(hydroxymethyl)-2,3-dihydroxypropyl)-1,4,7,10-tetraazacyclododecane tetrahydrochloride was first prepared. The compound was then reacted with chloroacetic acid at 70 ºC and pH 9-10 for 18 h. The yield was 65%. Gd-DO3A-butrol was then prepared by adding Gd_2_O_3_ to the ligand in water and stirring at 90 ºC for 6 h. Cation- and anion exchange resins were then added at room temperature, and the mixture was stirred for 30 min. The resins were recollected by filtration, and charcoal was added to the filtrate and refluxed for 1 h. The solution was filtered and evaporated to dryness. The residue was redissolved in water and ethanol, and then was refluxed for 2 h. Gd-DO3A-butrol was collected by filtration and drying under vacuum (12 h at 60 ºC). The yield was 87%. Mass spectroscopy (FAB) gave the following results: m/e 606 [(M + H)^+^]; m/e 1211 [(2M + H)^+^]. The infrared spectrum (KBr) had peakls at 3560, 3280, 2980, 2975, 2940, 2920, 2880, 2870, 1650, 1600, and 1380 cm−^1^. The structure was determined by X-ray crystallography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gadobutrol%20or%20Gd-DO3A-butrol%20or%20Gadovist%29%20AND%20in%20vitro)]

Pintaske et al. (18) determined the in vitro relaxivity of Gd-DO3A-butrol and other compounds (Gd-DTPA and Gd-BOPTA) in human plasma obtained from healthy volunteers. Measurements of Gd-DO3A-butrol in concentrations of 0.01 mM up to 64 mM at 37 ºC were made with 0.2−, 1.5−, and 3.0− Tesla (T) clinical scanners. The longitudinal relaxation rates (r_1_; liter х mmol−^1^ х s−^1^) of Gd-DO3A-butrol were 5.5 ± 0.3, 4.7 ± 0.2, and 3.6 ± 0.2, at 0.2, 1.5, and 3T, respectively. The transverse relaxation rates (r_2_; liter х mmol−^1^ х s−^1^) of were 10.1 ± 0.3, 6.8 ± 0.2, and 6.3 ± 0.3, at 0.2, 1.5, and 3 T, respectively. In comparison, these values were lower for Gd-DTPA but higher for Gd-BOPTA.

Vogler et al. (17) measured the in vitro physico-chemical properties of Gd-DO3A-butrol. The osmolality was found to be 0.57 osmol/kg for the 0.5 M concentration and 1.39 osmol/kg for the1 M concentration. The distribution coefficient (butanol/water) was 0.006, and the viscosity was 1.43 cP for the 0.5 M concentration and 3.7 cP for the 1 M concentration. The T_1_-relaxivity (liter х mmol−^1^ х s−^1^) in plasma was determined to be 5.6 at 0.45 T and 6.1 at 2 T. There was negligible protein binding of about 2.7% in plasma. With use of rat mast cells, the I_50_ (the concentration at which histamine was released) was found to be greater than 250 mM. The I_50_ value for lysozyme inhibition (the concentration at which 50% of the enzyme was inhibited) was greater than 300 mM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gadobutrol%20or%20Gd-DO3A-butrol%20or%20Gadovist%29%20AND%20rodentia)]

Vogler et al. (17) studied the long-term elimination and biodistribution of 0.25 mmol/kg Gd-DO3A-butrol in rats. More than 90% of the i.p. injected dose (ID) was excreted by the kidneys in 2 h and 100% in 7 days. The total amount remaining in the body decreased from 0.71% ID on day 1 to 0.15% ID on day 7 after injection. Inductively-coupled plasma atomic emission spectrometry (detection limit was 0.01 ppm or 65 nM) showed that only the kidneys, bones, and blood contained an amount of the agent above the detection limit after 7 days. The % ID of these organs were 0.06 ± 0.01, 0.01 ± 0.00, and 0.01 ± 0.00, respectively. The acute toxicity (lethal dose (LD_50_)) in mice was 23 mmol/kg. In a neural tolerance study, the median LD_50_ (lethal dose; n = 10) and effective dose (ED_50_) of Gd-DO3A-butrol in rats after intracisternal injection were 86 µmol/kg and 18 µmol/kg, respectively. In comparison, the LD_50_ and ED_50_ for Gd-DTPA were 740 µmol/kg and 73 µmol/kg, respectively. The study suggested that macrocyclic compounds had lower cerebral tolerance and that linear compounds had higher cerebral tolerance. Imaging studies in rat models with cerebral infarct, brain tumors, and intramuscular tumors showed contrast enhancements (0.3 mmol/kg Gd-DO3A-butrol) in all three pathologic areas. A dose-dependent increase in the signal intensity of the intramuscular tumors was observed.

Several rat studies (19-23) showed that Gd-DO3A-butrol was effective in providing contrast enhancement for MRI in glioma, brain ischemia, hepatocellular carcinoma, and the lymphatic system.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gadobutrol%20or%20Gd-DO3A-butrol%20or%20Gadovist%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Vogler et al. (17) performed Gd-DO3A-butrol pharmacokinetics studies in beagle dogs. The elimination t½ and the plasma clearance were 45 ± 3.6 min and 3.75 ± 0.30 ml/min/kg, respectively. The total volume of distribution at steady state (Vss) was 0.23 ± 0.02 liter/kg. High-performance liquid chromatography analysis of the plasma and urine samples showed that Gd-DO3A-butrol was not metabolized.

The abdominal MRI enhancement properties of Gd-DO3A-butrol were investigated in pigs (24). Images of 40 and 80 µmol/kg doses were conducted on a 1.5 T imager. Gd-DO3A-butrol gave signal intensity curves similar to those produced by extracellular agents. Significant enhancement was found in all tissues except the trunk muscles. Kalinoski et al. (25) used 1 M Gd-DO3A-butrol in a dose of 2 mmol/kg to demonstrate the feasibility of producing X-ray contrast enhancement with computed tomography (CT) in pigs

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Gadobutrol%20or%20Gd-DO3A-butrol%20or%20Gadovist%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28%22gadobutrol%22%5BSubstance%20Name%5D%20OR%20Gadobutrol%5BText%20Word%5D%29%20OR%20Gd-DO3A-butrol%5BAll%20Fields%5D%20OR%20%28%22gadolinium-DO3A-butriol%22%5BSubstan)]

Staks et al. (26) investigated the pharmacokinetics, dose proportionality, and tolerability of Gd-DO3A-butrol in healthy volunteers. Two double-blind, randomized, placebo-controlled phase I studies were conducted for testing a low concentration (0.5 M; doses = 0.04, 0.1, 0.2, 0.3, and 0.4 mmol/kg; n = 55) and a high concentration (1 M; doses = 0.3, 0.4, and 0.5 mmol/kg; n = 36). From the data for 24 volunteers, pharmacokinetic parameters were calculated from an open two-compartment model. The values for plasma elimination half-life (t_½p,β_;h), V_ss_ (liter/kg), renal clearance (ml/min/kg), and 72-h total renal excretion (Urine, 72 h (% ID)) for a 0.1 mmol/kg dose were 1.78 ± 0.43, 0.21 ± 0.02, 1.56 ± 0.18, and 98 ± 3.33, respectively. For a 0.4 mmol/kg dose, these values were 1.33 ± 0.21, 0.15 ± 0.02, 1.45 ± 0.22, and 96.6 ± 5.61, respectively. Plasma Gd-DO3A-butrol decreased bioexponentially, and the volume of distribution was within the extracellular fluid space. Elimination occurred primarily through the renal route. Biotransformation analysis of the urine and plasma samples revealed no metabolites from Gd-DO3A-butrol. No significant changes were observed in serum chemistry/hematology, or urine chemistry/urinalysis. No clear dose-dependent adverse events were found between the low-dose and high-dose studies. The most common adverse events were smell sensation (12.5%) and taste sensation (15%).

Tombach and Heindel (27) and Huppertz and Rohrer (28) summarized clinical studies for the clinical applications of 1 M Gd-DO3A-butrol. In 29 phase I to phsae III studies (2523 subjects and 2662 doses), Gd-DO3A-butrol was distributed in the extracellular fluid with a plasma terminal t½ of 1.7-2 h. Approximately 98% of the dose was excreted unchanged in the urine within 12 h. The studies indicated that 1 M Gd-DO3A-butrol had an excellent safety profile with doses ranging from 0.04 to 1.5 mmol/kg. Overall, 8.5% of the patients reported related and unrelated adverse events. For contrast enhancement, analysis of efficacy data showed results comparable to results to other commercially available 0.5 M Gd- chelates in studies of the CNS (677 patients), and angiography (676 patients).

In a study of the pharmacokinetics of 1 M Gd-DO3A-butrol in 21 patients with chronic renal failure, Tombach et al. (29) reported that the extracellular distribution of Gd-DO3A-butrol remained unchanged but the mean elimination t_½_ increased compared with that of healthy volunteers. Other human studies have shown the potential clinical usefulness of 1 M Gd-DO3A-butrol in various CNS and vascular diseases [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28gadovist%20OR%20Gadobutrol%20OR%20Gd-DO3A-butrol%20%29%20AND%20%28CNS%20OR%20angiography%20OR%20vascular%20diseases%29)].

## References

1 Pediconi F., Catalano C., Occhiato R., Venditti F., Fraioli F., Napoli A., Kirchin M.A., Passariello R. (2005). Breast lesion detection and characterization at contrast-enhanced MR mammography: gadobenate dimeglumine versus gadopentetate dimeglumine. Radiology.
2 Essig M. (2005). Gadobenate dimeglumine (MultiHance) in MR imaging of the CNS: studies to assess the benefits of a high relaxivity contrast agent. Acad Radiol.
3 Schlosser T., Hunold P., Herborn C.U., Lehmkuhl H., Lind A., Massing S., Barkhausen J. (2005). Myocardial infarct: depiction with contrast-enhanced MR imaging--comparison of gadopentetate and gadobenate. Radiology.
4 Tombach B., Reimer P. (2005). Soluble paramagnetic chelates and stabilized colloidal particle solutions of iron oxides as contrast agents for magnetic resonance imaging. Curr Med Chem.
5 Runge V., Kirsch J., Wells J., Awh M., Bittner D., Woolfolk C. (1993). Enhanced liver MR: Contrast agents and imaging strategy. Crit Rev Diagn Imaging.
6 DeSimone D., Morris M., Rhoda C., Lucas T., Zielonka J., Olukotun A., Carvlin M. (1991). Evaluation of the safety and efficacy of gadoteridol injection (a low osmolal magnetic resonance contrast agent). Clinical trials report. Invest Radiol.
7 Tweedle M. (1992). Physicochemical properties of gadoteridol and other magnetic resonance contrast agents. Invest Radiol.
8 Yuh W., Engelken J., Muhonen M., Mayr N., Fisher D., Ehrhardt J. (1992). Experience with high-dose gadolinium MR imaging in the evaluation of brain metastases. AJNR Am J Neuroradiol.
9 Tweedle M.F. (1997). The ProHance story: the making of a novel MRI contrast agent. Eur Radiol.
10 Vogler H., Platzek J., Schuhmann-Giampieri G., Frenzel T., Weinmann H.J., Raduchel B., Press W.R. (1995). Pre-clinical evaluation of gadobutrol: a new, neutral, extracellular contrast agent for magnetic resonance imaging. Eur J Radiol.
11 Platzek J., Blaszkiewicz P., Gries H., Luger P., Michl G., Muller-Fahrnow A., Raduchel B., Sulzle D. (1997). Synthesis and Structure of a New Macrocyclic Polyhydroxylated Gadolinium Chelate Used as a Contrast Agent for Magnetic Resonance Imaging. Inorg Chem.
12 Platzek J., Blaszkiewicz P., Gries H., Luger P., Michl G., Muller-Fahrnow A., Raduchel B., Sulzle D. (1997). Synthesis and Structure of a New Macrocyclic Polyhydroxylated Gadolinium Chelate Used as a Contrast Agent for Magnetic Resonance Imaging. Inorg Chem.
13. Product Monograph2004, 2004.
14 Perazella M.A., Rodby R.A. (2007). Gadolinium use in patients with kidney disease: a cause for concern. Semin Dial.
15 Grobner T., Prischl F.C. (2007). and Gadolinium and nephrogenic systemic fibrosis. Kidney Int.
16 Pedersen M. (2007). Safety update on the possible causal relationship between gadolinium-containing MRI agents and nephrogenic systemic fibrosis. J Magn Reson Imaging.
17 Vogler H., Platzek J., Schuhmann-Giampieri G., Frenzel T., Weinmann H., Raduchel B., Press W. (1995). Pre-clinical evaluation of gadobutrol: a new, neutral, extracellular contrast agent for magnetic resonance imaging. Eur J Radiol.
18 Pintaske J., Martirosian P., Graf H., Erb G., Lodemann K., Claussen C., Schick F. (2006). Relaxivity of Gadopentetate Dimeglumine (Magnevist), Gadobutrol (Gadovist), and Gadobenate Dimeglumine (MultiHance) in Human Blood Plasma at 0.2, 1.5, and 3 Tesla. Invest Radiol.
19 Fink C., Bock M., Kiessling F., Delorme S. (2002). Interstitial magnetic resonance lymphography with gadobutrol in rats: evaluation of contrast kinetics. Invest Radiol.
20 Frigeni V., Miragoli L., Grotti And A., Lorusso V. (2001). Comparative study between gadobenate dimeglumine and gadobutrol in rats with brain ischemia: evaluation of somatosensory evoked potentials. Invest Radiol.
21 Kawai J., Takahashi M., Kato N., Takashima K., Miyazawa T. (1999). Comparison of a 1.0 molar and a 0.5 molar formulation of gadobutrol in dynamic MR imaging of the liver in rats with hepatocellular carcinoma. Magn Reson Imaging.
22 Le Duc G., Corde S., Charvet A., Elleaume H., Farion R., Le Bas J., Esteve F. (2004). In vivo measurement of gadolinium concentration in a rat glioma model by monochromatic quantitative computed tomography: comparison between gadopentetate dimeglumine and gadobutrol. Invest Radiol.
23 Reimer P., Allkemper T., Bremer C., Rummeny E., Spiegel H., Balzer T., Peters P. (1997). Assessment of reperfusion injury by means of MR contrast agents in rat liver. J Magn Reson Imaging.
24 Adam G., Neuerburg J., Spuntrup E., Muhler A., Scherer K., Gunther R. (1994). Dynamic contrast-enhanced MR imaging of the upper abdomen: enhancement properties of gadobutrol, gadolinium-DTPA-polylysine, and gadolinium-DTPA-cascade-polymer. Magn Reson Med.
25 Kalinowski M., Kress O., Wels T., Alfke H., Klose K., Wagner H. (2003). 1-molar gadobutrol as a contrast agent for computed tomography: results from a comparative porcine study. Invest Radiol.
26 Staks T., Schuhmann-Giampieri G., Frenzel T., Weinmann H., Lange L., Platzek J. (1994). Pharmacokinetics, dose proportionality, and tolerability of gadobutrol after single intravenous injection in healthy volunteers. Invest Radiol.
27 Tombach B., Heindel W. (2002). Value of 1.0- M gadolinium chelates: review of preclinical and clinical data on gadobutrol. Eur Radiol.
28 Huppertz A., Rohrer M. (2004). Gadobutrol, a highly concentrated MR-imaging contrast agent: its physicochemical characteristics and the basis for its use in contrast-enhanced MR angiography and perfusion imaging. Eur Radiol.
29 Tombach B., Bremer C., Reimer P., Schaefer R., Ebert W., Geens V., Heindel W. (2000). Pharmacokinetics of 1M gadobutrol in patients with chronic renal failure. Invest Radiol.